# 2-[^18^F]Fluoropyridine-4-carbohydrazide-methotrexate

Chemical name: | 2-[^18^F]Fluoropyridine-4-carbohydrazide-methotrexate
Abbreviated name: | [^18^F]-Folate-MTX-9
Synonym: | [^18^F]-9
Agent Category: | Compound
Target: | Folate receptor
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on above structure for information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=folate%20receptor%20imaging&cmd=DetailsSearch)]

Folic acid (FA; also known as folate or vitamin B_9_) is a water-soluble vitamin that is required for the synthesis and repair of cellular DNA. FA also acts as a cofactor for many biological reactions and has an important role in cell maintenance and proliferation. Although the folate receptor (FR) is expressed at low levels in normal cells, this receptor is known to be upregulated in cancers such as those of the ovary, lung, breast, brain, colon, and the hematopoietic lineage cells (1). Therefore, the FR system has been targeted with radiolabeled folate and its derivatives, such as ^67^Ga-deferoxamine (DF)-folate, ^111^In-diethylenetriamine pentaacetic acid-folate, ^99m^Tc-mercaptoacetyldiglycine-folate-methotrexate, etc., for the noninvasive detection of malignancies with single-photon emission computed tomography (2). Mathias et al. showed that ^66/67^Ga-DF-folate can be used with positron emission tomography (PET) for the imaging of FR-positive cancerous tumors in mice (3). However, although these tracers could detect the FR-rich tumors, they were deemed unsuitable for imaging lesions in the abdominal regions because high levels of radioactivity were observed to accumulate in the liver and intestines of the animals (4). In addition, ^66/67^Ga-labeled tracers are known to produce low-resolution images because they generate high positron energy (4.15 MeV and 1.89 MeV for ^66^Ga and ^67^Ga, respectively) compared to ^18^F (0.64 MeV), which generates superior images and is often used to radiolabel PET imaging agents in the clinic (4). In another study, it was shown that ^18^F-fluorobenzylamine derivatives of folate could detect tumors that had a high expression of FR, but the radioactivity from these labeled compounds accumulated mainly at the rim of the tumor, and large amounts of the label were retained in the liver and intestines of the animals (4, 5).

In an ongoing effort to generate radiolabeled agents for the imaging of tumors that express high levels of FRs that would be superior to those developed and evaluated earlier, a ^18^F-fluorobenzene derivative of folic acid ([^18^F]-folate-1), a pyridinecarbohydrazide-folate derivative of folic acid ([^18^F]-folate-2), a ^18^F-fluorobenzene/methotrexate (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=78794e3d-f293-4eeb-22ac-8f536d5947eb) (MTX) conjugate of folic acid ([^18^F]-folate-MTX-8), and a ^18^F-pyridinecarbohydrazide-folate/methotrexate conjugate of folic acid ([^18^F]-folate-MTX-9) have been synthesized (2). The biodistribution of these tracers was investigated in healthy mice. On the basis of results obtained from these studies, [^18^F]-folate-2 was evaluated for the PET imaging of human KB cell line (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-17&Template=cellBiology) xenograft tumors (have a high expression of FR) in mice. This chapter describes the results obtained with [^18^F]-folate-MTX-9. Separate chapters in MICAD (www.micad.nih.gov) discuss the studies performed with [^18^F]-folate-1 (6), [^18^F]-folate-2 (7), and [^18^F]-folate-MTX-8 (8).

### Related Resource Links

FR-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Folate+receptor+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Adult human FR protein and mRNA sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_016724.2)

Human FR gene (http://www.ncbi.nlm.nih.gov/gene/2348) (Gene ID: 2348)

FR clinical trials (http://clinicaltrials.gov/ct2/results?term=folate+receptor+AND+targeted+AND+cancer)

FR in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/136430) database

FR pathway in Kyoto Encyclopedia of Genes and Genomes (KEGG) (http://www.genome.jp/dbget-bin/www_bget?hsa:2348+hsa:2350+hsa:2352+hsa:390243)

Folic acid information on Dailymed site (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=ff80ef4d-e04c-9f83-2b56-cccc30028f72)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20synthesis&cmd=DetailsSearch)]

Folate-MTX-9 was synthesized by the conjugation of the γ-isomer of N-succinimidyl-methotrexate carboxylate and 2-fluoropyridine-4-carbohydrazide in presence of triethylamine and Folate-MTX-8 were synthesized as described elsewhere (8). Both the compounds were labeled with ^18^F as described by Jammaz et al. (2). The synthesis and labeling of [^18^F]-folate-2 and [^18^F]-folate-1 have been detailed elsewhere (9). The total time of synthesis for each of the tracers was ~45 min, and the radiochemical yield and radiochemical purity of the final labeled products were >80% (based on the initial ^18^F concentration) and >97% (without high-performance liquid chromatographic purification), respectively. The specific activity of the different radiolabeled compounds was reported to be >11.11 MBq/μmol (300 mCi/μmol) (2).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20in%20vitro&cmd=DetailsSearch)]

Using an n-octanol-water mixture (pH 7.3), the partition coefficient of [^18^F]-folate-MTX-9 was determined to be 0.16 ± 0.01. The partition coefficients of [^18^F]-folate-1, [^18^F]-folate-2, and [^18^F]-folate-MTX-8 were reported to be 0.38 ± 0.02, 0.14 ± 0.01, and 0.43 ± 0.01, respectively, indicating that these labeled compounds had a low lipophilicity and that, among the three tracers, [^18^F]-folate-2 was least lipophilic (9).

[^18^F]-Folate-MTX-9, [^18^F]-folate-MTX-8, [^18^F]-folate-1, and [^18^F]-folate-2 were reported to be stable in human plasma for at least 4 h at 37°C (data not presented) (2).

From a saturation assay with KB cell membranes, the FR binding affinities of [^18^F]-folate-MTX-9, [^18^F]-folate-MTX-8, [^18^F]-folate-1, and [^18^F]-folate-2 were determined to be 31.42 ± 0.95 nM, 22.52 ± 1.79 nM, 13.08 ± 0.83 nM, and 15.51 ± 1.80 nM, respectively (9). A cell internalization assay of [^18^F]-folate-MTX-9, [^18^F]-folate-MTX-8, [^18^F]-folate-1, and [^18^F]-folate-2 with KB cells (using an acidic buffer, pH not mentioned) showed that 12.91 ± 0.58%, 23.42 ± 1.53%, 25.85 ± 0.95%, and 11.86 ± 0.43% of the tracers were respectively internalized by the cells within 20 min at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]-folate-MTX-9, [^18^F]-folate-MTX-8, [^18^F]-folate-1, and [^18^F]-folate-2 was studied in normal Balb/c mice as described by Jammaz et al. (2). The animals (n = 4 mice/time point for each tracer) were injected with 749 kBq (20 μCi) of the tracer through the tail vein and euthanized at 10, 60, and 120 min postinjection (p.i.) to determine the amount of radioactivity accumulated in the various organs. All data were presented as percent of injected dose per gram tissue (% ID/g). The radiotracer from [^18^F]-folate-MTX-9 was cleared rapidly from the blood (3.45 ± 0.42% ID/g at 10 min p.i., 3.24 ± 0.17% ID/g at 60 min p.i., and 1.51 ± 0.16% ID/g at 120 min p.i.). The kidneys showed a rapid clearance of radioactivity from [^18^F]-folate-MTX-9 (2.96 ± 0.59% ID/g at 10 min p.i. and 0.75 ± 0.26% ID/g at 120 min p.i.), but accumulation of the label in the intestines remained steady (3.54 ± 0.16% ID/g at 10 min p.i. and 3.37 ± 1.16% ID/g at 120 min p.i.). This indicated that the tracer was excreted through the urinary and the hepatobiliary routes in the animals. The label from [^18^F]-folate-MTX-8 was cleared rapidly from the blood (5.64 ± 0.95% ID/g at 10 min p.i., 1.90 ± 0.28% ID/g at 60 min p.i., and 1.08 ± 0.25% ID/g at 120 min p.i.). The kidneys accumulated high levels of radioactivity (8.93 ± 1.49% ID/g at 10 min p.i. and 6.40 ± 1.35% ID/g at 120 min p.i.), and a similar trend was noted with the intestine (6.33 ± 0.19% ID/g at 10 min p.i. and 7.17 ± 1.56% ID/g at 120 min p.i.). This indicated that the tracer was excreted through the urinary and the hepatobiliary routes in the animals. With [^18^F]-folate-1, rapid clearance of radioactivity from the blood was observed (4.41 ± 0.60% ID/g at 10 min p.i., 2.55 ± 1.50% ID/g at 60 min p.i., and 1.13 ± 0.51% ID/g at 120 min p.i.). High levels of label from [^18^F]-folate-1 were observed in the kidneys (22.50 ± 4.42% ID/g at 10 min p.i. and 17.88% ID/g ± 0.10 at 120 min p.i.) and the intestine (5.95 ± 2.11% ID/g at 10 min p.i. and 5.86 ± 0.26% ID/g at 120 min p.i.) of these animals, indicating that this tracer also was excreted through the urinary and the hepatobiliary routes. Radioactivity from [^18^F]-folate-2 was rapidly cleared from circulation (1.22 ± 0.61% ID/g at 10 min p.i., 0.10 ± 0.05% ID/g at 60 min p.i., and 0.04 ± 0.01% ID/g at 120 min p.i.). A high accumulation of label from [^18^F]-folate-2 was observed in the kidneys (13.8 ± 5.9% ID/g at 10 min p.i. and 2.92 ± 0.51% ID/g at 120 min p.i.), but the intestines accumulated a low level of the tracer (0.76 ± 0.20% ID/g at 10 min p.i. and 0.03 ± 0.01% ID/g at 120 min p.i.). This indicated that radioactivity from [^18^F]-folate-2 was excreted primarily through the urinary route. The accumulation of low levels of radioactivity with [^18^F]-folate-2 in the various organs suggested that this tracer had a superior pharmacokinetic profile compared to [^18^F]-folate-MTX-8 and [^18^F]-folate-1.

The biodistribution of [^18^F]-folate-MTX-9, [^18^F]-folate-MTX-8, [^18^F]-folate-1, and [^18^F]-folate-2 was also investigated in nude mice (n = 4 animals/tracer) bearing KB cell tumors (2). The animals were injected with the radiotracers as described above and euthanized at 60 min p.i. With all the radiolabeled compounds, the uptake of radioactivity in the various organs of the mice at 60 min p.i. was similar to that observed earlier (see above). The tumor uptake of label with [^18^F]-folate-MTX-9, [^18^F]-folate-MTX-8, [^18^F]-folate-1, and [^18^F]-folate-2 at 60 min p.i. was 1.00 ± 0.19% ID/g, 0.81 ± 0.09% ID/g, 5.94 ± 1.16% ID/g, and 5.74 ± 0.16% ID/g, respectively, indicating that the tumor uptake of radioactivity with [^18^F]-folate-MTX-9 and [^18^F]-folate-MTX-8 was significantly lower (P < 0.05) than that observed with either [^18^F]-folate-1 or [^18^F]-folate-2. The tumor/blood and tumor/muscle ratios with [^18^F]-folate-MTX-9, [^18^F]-folate-MTX-8, [^18^F]-folate-1, and [^18^F]-folate-2 at 60 min p.i. were 0.90 and 1.80, 0.80 and 1.63, 6.39 and 25.83, and 14.70 and 28.70, respectively.

For blocking studies, the mice were injected with 100 μg (0.22 μmol) FA 10 min before the administration of [^18^F]-folate-MTX-9, [^18^F]-folate-MTX-8, [^18^F]-folate-1, or [^18^F]-folate-2, and the rodents were subsequently treated as before (2). With [^18^F]-folate-MTX-9 and [^18^F]-folate-MTX-8, the tumors showed a significantly reduced (P < 0.05) uptake of radioactivity (0.28 ± 0.13% ID/g and 0.19 ± 0.10% ID/g, respectively) at 60 min p.i., and a similar trend was evident in the kidneys, intestines, and liver. The tumors showed a significantly reduced accumulation of radioactivity (0.74 ± 0.17% ID/g, P < 0.05) with [^18^F]-folate-1 at 60 min p.i., and the kidneys, liver, and the intestines (among these organs the kidney and the liver express higher levels of FR compared with other normal tissues) of the animals also showed reduced levels of the label (P < 0.05). With [^18^F]-folate-2, the uptake of radioactivity in the tumor at 60 min p.i. was reduced to 0.66 ± 0.10% ID/g (P < 0.05), and a similar trend was observed in the kidneys, liver, and intestines (P < 0.05). These studies indicated that all of these ^18^F-labeled folate derivatives had good binding specificity for the FR in the tumors and various organs of the animals.

Table: Tumor Uptake and Tumor/Blood and Tumor/Muscle Ratios of Different ^ 18 ^ F-Labeled Folate and Folate-MXT Compounds

Tracer | Tumor Uptake (% ID/g) | | Ratio
Tracer | No Folate Pretreatment | With Folate (100 μg) Pretreatment | Tumor/Blood | Tumor/Muscle
[ ^ 18 ^ F]-Folate-1 | 5.94 ± 1.16 | 0.74 ± 0.17 | 6.39 | 25.83
[ ^ 18 ^ F]-Folate-2 | 5.74 ± 0.16 | 0.66 ± 0.10 | 14.72 | 28.70
[ ^ 18 ^ F]-Folate-MXT-8 | 0.18 ± 0.09 | 0.19 ± 0.10 | 0.90 | 1.80
[ ^ 18 ^ F]-Folate-MXT-9 | 1.00 ± 0.19 | 0.28 ± 0.13 | 0.80 | 1.63

From the studies and the results discussed above, the investigators concluded that [^18^F]-folate-2 was probably superior to [^18^F]-folate-MTX-9, [^18^F]-folate-MTX-8, and [^18^F]-folate-1 for the imaging of FR-expressing tumors in rodents (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Xia W., Low P.S. (2010). Folate-targeted therapies for cancer. J Med Chem.
2 Al Jammaz I., Al-Otaibi B., Amer S., Okarvi S.M. (2011). Rapid synthesis and in vitro and in vivo evaluation of folic acid derivatives labeled with fluorine-18 for PET imaging of folate receptor-positive tumors. Nucl Med Biol.
3 Mathias C.J., Lewis M.R., Reichert D.E., Laforest R., Sharp T.L., Lewis J.S., Yang Z.F., Waters D.J., Snyder P.W., Low P.S., Welch M.J., Green M.A. (2003). Preparation of 66Ga- and 68Ga-labeled Ga(III)-deferoxamine-folate as potential folate-receptor-targeted PET radiopharmaceuticals. Nucl Med Biol.
4 Sega E.I., Low P.S. (2008). Tumor detection using folate receptor-targeted imaging agents. Cancer Metastasis Rev.
5 Bettio A., Honer M., Muller C., Bruhlmeier M., Muller U., Schibli R., Groehn V., Schubiger A.P., Ametamey S.M. (2006). Synthesis and preclinical evaluation of a folic acid derivative labeled with 18F for PET imaging of folate receptor-positive tumors. J Nucl Med.
6 Chopra, A., 2-[(4-{[(2-amino-4-oxohydropteridin-7yl)methyl]amino}phenyl) carbonylamino]-4-{N-[(4-[18F]-fluorophenyl)carbonylamino] carbamoyl}butanoic acid. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
7 Chopra, A., 2-[(4-{[(2-amino-4-oxohydropteridin-7yl)methyl]amino}phenyl) carbonylamino]-4-{N-[(2-[18F]-fluoro(4-pyridyl))carbonylamino] carbamoyl}butanoic acid. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
8 Chopra, A., 4-[18F]Fluorobenzencarbohydrazide-methotrexate (8). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
9 Jammaz I.A., Otaibi B.A., Okarvi S., Amartey J.K. (2006). Novel synthesis of [18F]-fluorobenzene and pyridinecarbohydrazide-folates as potential PET radiopharmaceuticals. Journal of Labelled Compounds and Radiopharmaceuticals.